# Luciferase-expressing Escherichia coli

Chemical name: | Luciferase-expressing Escherichia coli
Abbreviated name: | pLux-expressing E. coli
Synonym: | Light-emitting E. coli
Agent Category: | Escherichia coli
Target: | Non-specific tumor
Target Category: | Bioluminescence
Method of detection: | Optical imaging
Source of signal: | Bioluminescence luciferase-expressing plasmid pLux
Activation: | Yes
Studies: | - In vitro; - Rodents | Click for the nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=161344133) sequence and the amino acid sequence of subunit A (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=161344134) and subunit B (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=161344135) of Photobacterium leiognathi luciferase.

## Background

[PubMed] (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=+bacterial+targeted+tumor+therapy+&WebEnv=0TjBtYBfT1BFtKYfekyJ04ZxEQ7W677it4mVYOmkb5q21GjfLb4mHzSAIrebyg2ebr-4xPFCtYIvM8J%407748428072881B60_0000SID&WebEnvRq=1)

A variety of therapies such as radiation, chemotherapy, recombinant biological drugs, surgical resection, or a combination of these regimens may be, and often are, used to treat neoplastic conditions. However, although promising to some extent, none of these treatments assures a successful outcome for the patient. It is also known that early detection and treatment of cancer greatly improves the odds of a favorable outcome. Therefore, medical researchers and professionals have devoted much effort to the development of different techniques and modalities such as positron emission tomography, single-photon emission computed tomography, magnetic resonance imaging, ultrasound, etc., for the detection and diagnosis of cancers (1-4).

Interestingly, the detection of different bacteria in tumors removed from patients has been documented, and some investigators have attempted to use the bacteria as a means to detect and target neoplastic tumors (5, 6). The bacteria appear to accumulate, survive, and thrive under the hypoxic and necrotic conditions found in the tumors, whereas they do not grow in normal tissues that have a rich supply of oxygen (7). The spores of an anaerobic strain of Clostridium novyi, created by removing the lethal toxin gene in the bacteria, germinated in the avascular regions of the tumor and subsequently destroyed the tumor cells (7). In addition, the ability of these bacteria to accumulate and grow in tumors has been exploited by using them as a signal source to image tumors (8). To achieve this, the bacteria were genetically engineered to express luciferase (Lux) or green fluorescence protein (GFP) genes and used to target and visualize tumors in mice (8). By engineering the luxCDABE gene cluster into the bacteria, a continuous light-emitting microbe was generated that did not need an external stimulus or substrate for the emission of light (8, 9). The emission of light is an energy-dependent process, the mechanism of which has been detailed elsewhere (10).

The use of Salmonella typhimurium for the treatment of cancers has been evaluated in clinical trials (http://clinicaltrials.gov/ct2/results?term=Salmonella+typhimurium) approved by the United States Food and Drug Administration (11, 12)

This chapter briefly describes the use of Escherichia coli transduced with a pLux plasmid that expresses the luciferase gene for the imaging of xenograft tumors in mice (13). After intravenous administration of the pLux-expressing E. coli, bioluminescence from the microbes could be detected exclusively in the tumor tissue 24 h later.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=light+emitting+bacteria&WebEnv=0lD5Q5FH3MCyF-7DIEFC9-fSbYsk4kuO9t2h2oD0GqfrI9qIm44FFcEPb2rXTqK0xmtWIbTLR_avK11%407748428072881B60_0000SID&WebEnvRq=1)]

The E. coli strains MG1655 and HJ1020 and the plasmids used for this study were as described by Min et al. (13). The bacterial strains were generated by using the P1 transduction protocol as described by Silhavy et al. (14). The E. coli strain HJ1020 (asd::kan) was constructed from MG1655 as detailed elsewhere (15). The asd open reading frame in the plasmid pKD13 was replaced with kan by polymerase chain reaction (PCR) amplification with the use of appropriate primers. Subsequently, kan was removed to generate ∆asd as described by Datsenko and Wanner (15). The pLux plasmid was constructed by ligating a 9.5-kb XbaI fragment from pT7-3-Lux (a plasmid that contains the luxCDABE sequence obtained from Photobacterium leiognathi (16)) into the same site in the pUC19 plasmid so the lux operon could be driven by the lac promoter.

To construct the plasmid containing the dual Lux and asd cassette, the asd gene was PCR-amplified from E. coli MG1655, and the 1.1-kb fragment was cloned into the plasmid pGEM-T Easy that had been digested with EcoRI and ligated into the same site in pLux to generate the Asd^+^ pLux construct (13). The asd gene codes for aspartate β-semialdehyde dehydrogenase, and to survive the E. coli asd mutants have an obligate requirement for diaminopimelic acid, without which the cells are lysed. Therefore, bacterial cells containing the Asd^+^ pLux construct would be expected to survive longer compared to those harboring only the pLux plasmid.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=light+emitting+bacteria+in+vitro+studies&WebEnv=0-X3DVIzZflHOgWk_0n8slR1RuvKFE_dFx9aka67Rp_5xPyf6KUkbum0JSwIQ7Zi42DlHOA9BA2uuD%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=light+emitting+bacteria+rodentia&WebEnv=0STfB7KO2UMael-Iyjy3tQFwx1JdZjvF7REwjZmIc-H7i8W6ovUKt6PcDa4oUtRkY0ELDTzHBI3DWz%407748428072881B60_0000SID&WebEnvRq=1)]

Tumors were visualized with the use of light-emitting E. coli in BALB/c and BALB/c athymic nu-/nu- mice bearing subcutaneous tumors generated with CT26 (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=CRL-2638), C6 (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=CCL-107), SNU-C5 (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=CRL-5972) and B16-F10 (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=CRL-6475) cells in the thigh or right shoulder of each animal (13). To determine the optimal number of bacterial cells necessary for noninvasive imaging, different numbers of E. coli were injected subcutaneously into mice bearing tumors and the bioluminescence signals were acquired. The minimum number of E. coli required for imaging was determined to be 10^4^, and the signal correlated well for up to 10^9^ bacteria administered to the animals.

The biodistribution of E. coli that expresses the lux gene was determined in the mice bearing CT26 cell tumors (13). The distribution of E. coli carrying either the pLux or the Asd^+^ pLux in nude mice (n > 6) was investigated. The animals were infected by an intravenous injection of 10^8^E. coli through the tail vein, and whole-body images were acquired. During the first few hours the signal was detected primarily in the liver and spleen of the animals, but by 24 h the signal was reduced in these organs and was detected exclusively in the tumor region of the animals. The investigators reported that the bioluminescence of the bacteria containing the pLux plasmid in the tumor peaked by day 4, and it decreased to undetectable levels after that time (probably because of a loss of the plasmid from the cells). However, tumors with E. coli containing the Asd^+^ pLux plasmid maintained the bioluminescence levels for up to 20 days after inoculation. The bacterial numbers in the normal tissue and the tumors were determined to investigate any correlation between the bacterial number and imaging. Presence of the bacteria in the tissue was confirmed by growing serial dilutions of tissue homogenates on agar plates containing ampicillin. Immediately after inoculation with the bacteria, the highest bacterial count was evident in the spleen, liver, and lungs of the animals (2.0 × 10^4^/g tissue to 1.6 × 10^7^/g tissue) with a low count in the tumor (9.5 × 10^2^/g tissue), but within 24 h the number of bacteria in the tumor increased >1,000-fold, reaching ~10^8^/g tissue by day 4 after inoculation. During the same period the number of bacteria in the spleen, liver, and lungs decreased, and the bacteria were undetectable in these organs at day 4. This indicated that the bacteria were cleared from the normal organs but accumulated and proliferated in the tumors.

Confocal microscopic examination of the tumor tissue revealed that the E. coli bacteria were present between the central necrotic part and the peripheral proliferative region of the lesion, but they were not detected in the peripheral proliferative region of the tumor (13). The investigators reported observing a higher number of tumor necrosis cases in the infected versus in the uninfected mice, and Min et al. suggested that the intravenously injected bacteria spread from the central necrotic region of the tumor to the peripheral regions.

The bioluminescent bacteria were observed to accumulate in a variety of tumors regardless of size, location (subcutaneous, intracecal, or shoulder, etc.), or immune status because the tumors could be detected both in the nude and the immunocompetent mice (13). In addition, the bacteria were observed to accumulate in the tumors whether administered through an intravenous or by an intraperitoneal inoculation.

In another study, the investigators established a metastatic tumor model in mice using the 4T1 (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=CRL-2539) murine breast cancer cells that metastasize specifically to the liver and the lungs (13, 17). As a control, a 4TO7 murine breast cancer cell line that does not metastasize was used to produce tumors. The cells were injected into the right fat pads of the BALB/c mice to establish an orthotopic breast cancer and metastasis (13). Four weeks after injection, E. coli Asd^+^ pLux were intravenously injected into the animals, and the bioluminescence signal was traced for three days. Immediately after inoculation, bacterial bioluminescence was detected in the liver for both tumor types. By two days after inoculation, the bioluminescence was also detected in the primary tumor sites (fat pads in the abdomen), but only the mice carrying the metastatic 4T1 tumor cells exhibited continuing bioluminescence in the liver, which indicates the presence of metastasis in the organ (13). The metastasis was confirmed by a histological examination, and such lesions were absent from the liver of control animals. From these observations the investigators concluded that bioluminescent E. coli is capable of imaging both primary and metastatic cancers (13).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=light+emitting+bacteria+non+primate+mammals&WebEnv=0ngNdta-UcGUgiuJqI_5f-LHOqkvbsl9rcbf-mB3JAmoVsIlo-Q8GDfQ_TpPatsnO9bC2zLPho-d6Nv%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=light+emitting+bacteria+non+human+primates&WebEnv=00R1EsoCPkcSufNhzvLe98SpHEG1Az2J0vKuHsoD1BS4BOb9LxBL9Aoa8HD9_GE3x3zl-pEmWgGXDo0%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=light+emitting+bacteria+human+studies&WebEnv=0kVniuEEFHxPd4VHriWK0OskjuNgXRFonNiLTZMKXFOb2BCyFnviZ32RkMFi0H1FWb6o8PEvTikOzM1%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Chong S., Lee K.S. (2007). Spectrum of findings and usefulness of integrated PET/CT in patients with known or suspected neuroendocrine tumors of the lung. Cancer Imaging.
2 Stillebroer A.B., Oosterwijk E., Oyen W.J., Mulders P.F., Boerman O.C. (2007). Radiolabeled antibodies in renal cell carcinoma. Cancer Imaging.
3 Richards P.S., Peacock T.E. (2007). The role of ultrasound in the detection of cervical lymph node metastases in clinically N0 squamous cell carcinoma of the head and neck. Cancer Imaging.
4 Morana G., Salviato E., Guarise A. (2007). and , Contrast agents for hepatic MRI. Cancer Imaging, . 7 Spec No A: p. S24-7.
5 Pawelek J.M., Low K.B., Bermudes D. (2003). Bacteria as tumour-targeting vectors. Lancet Oncol.
6 Wei M.Q., Mengesha A., Good D., Anne J. (2008). Bacterial targeted tumour therapy-dawn of a new era. Cancer Lett.
7 Dang L.H., Bettegowda C., Huso D.L., Kinzler K.W., Vogelstein B. (2001). Combination bacteriolytic therapy for the treatment of experimental tumors. Proc Natl Acad Sci U S A.
8 Yu Y.A., Timiryasova T., Zhang Q., Beltz R., Szalay A.A. (2003). Optical imaging: bacteria, viruses, and mammalian cells encoding light-emitting proteins reveal the locations of primary tumors and metastases in animals. Anal Bioanal Chem.
9 Fernandez-Pinas F., Wolk C.P. (1994). Expression of luxCD-E in Anabaena sp. can replace the use of exogenous aldehyde for in vivo localization of transcription by luxAB. Gene.
10 Thorn R.M., Nelson S.M., Greenman J. (2007). Use of a bioluminescent Pseudomonas aeruginosa strain within an in vitro microbiological system, as a model of wound infection, to assess the antimicrobial efficacy of wound dressings by monitoring light production. Antimicrob Agents Chemother.
11 Toso J.F., Gill V.J., Hwu P., Marincola F.M., Restifo N.P., Schwartzentruber D.J., Sherry R.M., Topalian S.L., Yang J.C., Stock F., Freezer L.J., Morton K.E., Seipp C., Haworth L., Mavroukakis S., White D., MacDonald S., Mao J., Sznol M., Rosenberg S.A. (2002). Phase I study of the intravenous administration of attenuated Salmonella typhimurium to patients with metastatic melanoma. J Clin Oncol.
12 Nemunaitis J., Cunningham C., Senzer N., Kuhn J., Cramm J., Litz C., Cavagnolo R., Cahill A., Clairmont C., Sznol M. (2003). Pilot trial of genetically modified, attenuated Salmonella expressing the E. coli cytosine deaminase gene in refractory cancer patients. Cancer Gene Ther.
13 Min J.J., Kim H.J., Park J.H., Moon S., Jeong J.H., Hong Y.J., Cho K.O., Nam J.H., Kim N., Park Y.K., Bom H.S., Rhee J.H., Choy H.E. (2008). Noninvasive Real-time Imaging of Tumors and Metastases Using Tumor-targeting Light-emitting Escherichia coli. Mol Imaging Biol.
14 Silhavy T.J., Berman M.L., Enquist L.W. (1984). and , Experiments with gene fusion. , Cold Spring Harbour Laboratory Press.: New York.
15 Datsenko K.A., Wanner B.L. (2000). One-step inactivation of chromosomal genes in Escherichia coli K-12 using PCR products. Proc Natl Acad Sci U S A.
16 Lee C.Y., Szittner R.B., Meighen E.A. (1991). The lux genes of the luminous bacterial symbiont, Photobacterium leiognathi, of the ponyfish. Nucleotide sequence, difference in gene organization, and high expression in mutant Escherichia coli. Eur J Biochem.
17 Aslakson C.J., Miller F.R. (1992). Selective events in the metastatic process defined by analysis of the sequential dissemination of subpopulations of a mouse mammary tumor. Cancer Res.